# Indocyanine green-polyethylene glycol-folate

Chemical name: | Indocyanine green-polyethylene glycol-folate
Abbreviated name: | fPI-01
Synonym: | Folate-PEG-ICG-Der-01
Agent category: | Compound
Target: | Folate receptor
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Indocyanine green (ICG)
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fPI-01)]

Optical fluorescence imaging is increasingly used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350-700 nm) are used. Near-infrared (NIR) fluorescence (700-1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive complement to radionuclide imaging in small animals.

Folic acid is a water-soluble B vitamin (4) that is essential for methylation and DNA synthesis. The primary pathway for folate entry into cells is through the facilitated transporter, which has a low affinity for folate (Michaelis constant (K_m_) = 1–5 μM). Some cells in the choroid plexus, kidney, lung, thyroid, spleen, placenta, and thymus also possess a higher-affinity receptor (dissociation constant (K_d_) = 0.5 nM) that allows folate uptake via receptor-mediated endocytosis. Some human epithelial tumor cells were found to overexpress folate-binding protein (5). More than 90% of human ovarian and endometrial cancers express the high-affinity receptor, which is absent in the respective normal tissues. Breast, colorectal, renal, and lung carcinomas also overexpress the folate receptor but at lower frequencies (20%–50%). Activated macrophages, but not resting macrophages, have also been found to have folate receptor (6). Several folate-based conjugates have been studied in tumor imaging [PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%28%22folic%20acid%22%5BMeSH%20Terms%5D%20OR%20%28%22folic%22%5BAll%20Fields%5D%20AND%20%22acid%22%5BAll%20Fields%5D%29%20OR%20%22folic%20acid%22%5BAll%20Fields%5D%20OR%20%22folate%22%5BAll%20Fields%5D%29%20AND%20%28%22Receptor%22%5BJournal%5D%20OR%20%22receptor%22%5BAll%20Fields%5D%29%20AND%20%28%22molecular%20imaging%22%5BMeSH%20Terms%5D%20OR%20%28%22molecular%22%5BAll%20Fields%5D%20AND%20%22imaging%22%5BAll%20Fields%5D%29%20OR%20%22molecular%20imaging%22%5BAll%20Fiel)].

Lin et al. (7) reported the synthesis of four new, water-soluble, NIR cyanine fluorophores that have superior chemical stability and optical properties. One of the NIR dyes (NIR2) was conjugated to amino-derivatized folic acid to form NIR2-folate, which has an excitation maximum at 665 nm and an emission maximum at 686 nm. NIR2-folate is being developed as an optical imaging agent for detection of folate receptors in vivo. Among the various NIR agents, only indocyanine green (ICG), with absorption at 780 nm and emission at 820 nm, is approved by the United States Food and Drug Administration for clinical applications in angiography, blood flow evaluation, and liver function assessment (8). It is also under evaluation in several clinical trials (http://clinicaltrials.gov/ct2/results?term=indocyanine+green) for other applications. Liu et al. (9) conjugated a hydrophobic derivative of ICG (ICG-Der-01) to the ɣ-carboxyl group of folic acid using PEG-bis-amine (4 kDa) as a linker to form folate-PEG-ICG-Der-01 (fPI-01) for in vivo NIR imaging of tumors in mice.

### Related Resource Links:

- Chapters in MICAD (Folate (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=folate+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (Folate receptor (http://www.ncbi.nlm.nih.gov/gene/2348))
- Articles in Online Mendelian Inheritance in Man (OMIM) (Folate receptor (http://www.ncbi.nlm.nih.gov/omim/136430))
- Clinical trials (Folate receptor (http://www.clinicaltrials.gov/ct2/results?term=folate+receptor), ICG (http://www.clinicaltrials.gov/ct2/results?term=ICG))
- Drug information in FDA (Folate receptor (http://google2.fda.gov/search?q=folate+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=15), ICG (http://google2.fda.gov/search?q=Indocyanine+Green&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=4&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fPI-01%20and%20synthesis)]

Liu et al. (9) prepared folate-PEG-amine by reaction of folic acid with PEG-bis-amine in anhydrous dimethyl sulfoxide (DMSO) with diisopropylcarbodiimide/N-hydroxysuccinimide (DCC/NHS). Folate-PEG-amine was purified with column chromatography. A mixture of ICG-Der-01, DCC, and NHS (molar ratio, 1:1.2:2.2) in DMSO was incubated for 2 h at room temperature to form ICG-Der-01-NHS. A solution of folate-PEG-amine and ICG-Der-01-NHS (molar ratio, 1:2) in carbonate buffer (pH 9) was stirred for 8 h at room temperature to produce fPI-01. fPI-01 was purified with column chromatography. Absorption and fluorescence spectra of fPI-01 demonstrated characteristics of both folic acid and ICG-Der-01. fPI-01 exhibited an excitation peak at 765.9 nm and an absorption peak at 783 nm, and fPI-01 was more photostable than ICG-Der-01.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fPI-01%20and%20in%20vitro)]

Human hepatoma cell line Bel-7402, epithelial cervical cancer cell line HeLa, and hepatocellular liver carcinoma HepG2 cells express high levels of mRNAfor folate receptor, whereas cells from the human lung carcinoma A549 have no detectable level (9). HeLa and A549 cells were incubated with 62.5–2,000 nM fPI-01 for 90 min. The NIR signal from HeLA cells was ~50% higher than that from A549 cells at the same concentration.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fPI-01%20and%20rodentia)]

Liu et al. (9) performed a series of whole-body NIR fluorescence imaging in normal nude mice (n = 4) and nude mice bearing Bel-7402 or A549 tumors (n = 4) after intravenous injection of 2 nmol fPI-01. In normal nude mice, the fluorescence signal was visualized mainly in the liver at 10 min after injection. There was a decrease in signal in the liver and an increase in signal in the urinary bladder at 30 min and 60 min. Ex vivo examination of the internal organs showed that strong signal could be seen in the liver, kidney, and urinary bladder but not in the heart, lung, spleen, or intestines at 8 h after injection. In Bel-7402 tumor-bearing mice, fPI-01 accumulated mainly in the tumor, liver, and urinary bladder at 2 h after injection. The tumor/background ratio was 20 at 4 h. The tumor was still visualized at 48 h, whereas the liver and urinary bladder were barely visualized. On the other hand, ICG-Der-01 accumulated mainly in the liver and intestines at 10 s, 2 h, and 4 h after injection. No signal was detected in the tumor at these time points. In A549 tumor-bearing mice, fPI-01 accumulated mainly in the liver and urinary bladder at 1–24 h after injection. The folate receptor-negative A549 tumors were barely visualized during 24 h of imaging. No blocking studies were performed to assess specificity of fPI-01 though folate receptor negative tumor was studied.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fPI-01%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fPI-01%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=fPI-01%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Stanger O. (2002). Physiology of folic acid in health and disease. Curr Drug Metab.
5 Ke C.Y., Mathias C.J., Green M.A. (2003). The folate receptor as a molecular target for tumor-selective radionuclide delivery. Nucl Med Biol.
6 Nakashima-Matsushita N., Homma T., Yu S., Matsuda T., Sunahara N., Nakamura T., Tsukano M., Ratnam M., Matsuyama T. (1999). Selective expression of folate receptor beta and its possible role in methotrexate transport in synovial macrophages from patients with rheumatoid arthritis. Arthritis Rheum.
7 Lin Y., Weissleder R., Tung C.H. (2002). Novel near-infrared cyanine fluorochromes: synthesis, properties, and bioconjugation. Bioconjug Chem.
8 Sakka S.G. (2007). Indocyanine green plasma disappearance rate as an indicator of hepato-splanchnic ischemia during abdominal compartment syndrome. Anesth Analg.
9 Liu F., Deng D., Chen X., Qian Z., Achilefu S., Gu Y. (2010). Folate-polyethylene glycol conjugated near-infrared fluorescence probe with high targeting affinity and sensitivity for in vivo early tumor diagnosis. Mol Imaging Biol.